# ^123^I-Annexin V

Chemical name: | ^123^I-Annexin V
Abbreviated name: | ^123^I-Anx5
Synonym: | ^123^I-rh-Anx5, ^123^I-labeled human recombinant annexin V, ^123^I-rh-annexin V, ^125^I-Anx A5
Agent Category: | Protein
Target: | Phosphatidylserine (PS)
Target Category: | Receptor binding
Method of detection: | Single-Photon Emission Computed Tomography (SPECT), gamma planar imaging
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=430966), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4809273) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=308) for more information about Annexin V

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29)]

^123^I-Annexin V (^123^I-Anx5) is a radioiodinated protein molecule developed for single-photon emission computed tomography (SPECT) imaging of programmed cell death (apoptosis) (1, 2). ^123^I is a gamma emitter with a physical t_½_ of 13.2 h.

Apoptosis is an essential biological process that maintains homeostasis of tissues and organs in concert with proliferation, growth, and differentiation (3, 4). Cell death can occur by the process of necrosis or by the process of apoptosis. Apoptosis is a highly regulated, genetically controlled, noninflammatory process requiring ATP (5). The apoptotic process can be triggered either by a decrease in factors required to maintain the cell in good health or by an increase in factors that cause cells to die (6). The two known mechanisms of apoptosis are the death receptor (extrinsic) and the mitochondrial (intrinsic) pathways (7). Annexin V (Anx5) is one of the numerous members of the calcium- and phospholipids-binding superfamily of annexin proteins. The mature Anx5 molecule consists of 319 amino acids with a total molecular weight of 35.8 kDa. Most of the biological functions of Anx5 are based on its high affinity for negatively charged phospholipids in the presence of physiologic concentrations of calcium. Anx5 binds to membrane-bound phophatidylserine (PS) which is normally restricted to the inner leaflet of the plasma membrane lipid bilayer (6). PS is exposed on the surfaces of cells as they undergo apoptosis. This change in the membrane can be detected by the binding of Anx5 to the external PS (7-9). It is also possible that Anx5 binds to PS exposed on the cell surface in pathologic conditions associated with necrosis and vascular damage.

Anx5 has been labeled with various radionuclides for SPECT and positron emission tomography imaging of apoptosis (7, 10). The detection of cell death in vivo has potential clinical value for possible diagnosis and assessment of therapeutic efficacy in transplanted organ rejections, AIDS, septic shock, cardiovascular diseases, neurodegenerative disorders, and cancer. Anx5 was originally obtained from human tissue. Currently, recombinant human Anx5 (rh-Anx5) can be produced in high yields with excellent purity by bioengineering techniques. Direct radioiodination of Anx5 proteins has been performed by means of electrophilic aromatic substitution of the molecule’s tyrosine residues (1). Alternatively, Anx5 has also been radioiodinated indirectly using prelabeled reagents (11). Because of their structural similarity to thyroxine, the directly iodinated proteins are more likely to exhibit in vivo deiodination than the indirectly iodinated proteins (12).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20synthesis)]

Tait et al. (13) prepared ^123^I-Anx5 using Anx5 purified from human placenta with ≥99% purity. Radiolabeling was done by the direct radioiodination method using 1,3,4,6-tetrachloro-3,6-diphenyl-glycoluril (Iodo-Gen). Anx5 protein was combined with Na^123^I in a Tris buffer (pH 8.0) in a glass tube coated with Iodo-Gen. After incubation for 15 min at room temperature, the reaction was quenched with sodium metasulfite, and excess Na^123^I was removed by gel filtration. The specific activity was 56,500 cpm/ng, and the labeling efficiency was 99.2−99.9%. Using the same radioiodination method, ^125^I-Anx5 (specific activity = 7480-14100 cpm/ng) fully retained its phospholipids- and human platelets-binding.

Lahorte et al. (1) reported the synthesis of ^123^I-rh-Anx5 (recombinant human Anx5) by the Iodo-Gen method. Briefly, Iodo-Gen−coated Eppendorf vials were prepared by evaporation of an Iodo-Gen solution at a concentraton of 60 μg/200 μl. The best result was obtained with 5 μg rh-Anx5 in 40 μl potassium phosphate (KH_2_PO_4_) buffer (0.1 M, pH 8) at ambient temperature (18ºC) for 10 min. The final product was purified by high-performance liquid chromatography. The radiochemical yield was 70% with >95% radiochemical purity. The specific activity was 7.4-92.5 MBq/μg.(0.2−2.5 mCi/μg).

To prepare clinical grade ^123^I-rh-Anx5 (recombinant human Anx5), Lahorte et al. (2) used a modified IodoGen method. In this method, 250 μg/ml of freshly prepared IodoGen in 2 ml was evaporated under a gentle stream of nitrogen in a 10-ml reaction vial. The vial was washed twice with 2 ml 0.05 M phosphate-buffered saline (PBS) before use. Then 1 mg of rh-Anx5 in 0.05 M PBS (pH 7.4) was mixed with 370 MBq (10 mCi) ^123^I in 0.5 M PBS (volume twice that of ^123^I) and incubated with gentle stirring at room temperature for 20 min. The reaction was stopped by purification on a PD10(G25) Sephadex column using 0.25% human serum albumin PBS as eluent. The final product was filtered by a 0.22-μm sterile filter. The radiochemical yield was 87.0 ± 6.5% with >98% radiochemical purity. The specific activity of ^123^I-rh-Anx5 was 13,400 MBq/μmol (362 mCi/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20in%20vitro)]

Lahorte et al. (1) used human platelets to determine whether ^123^I-rh-Anx5 maintained its biological activity. Isolated human platelets (108 cells/ml) were incubated with ^123^I-rh-Anx5 at ambient temperature for 30 min in the presence of various Ca^2+^ concentrations. The binding of ^123^I-rh-Anx5 to human platelets showed a Ca^2+^ -dependent response that reached a plateau of 67% at 20 mM Ca^2+^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20rodentia)]

Lahorte et al. (2) studied the acute toxicity of rh-Anx5 in mice. All mice showed few signs of adverse effects with 0.335, 1.342 or 2.685 mg/kg of decayed, clinical-grade ^123^I-rh-Anx5 in a single i.v. dose.

The biodistribution of ^123^I-rh-Anx5 was studied in mice (2). Each mouse received 74.0 ± 3.7 kBq (2 ± 0.1 μCi) of ^123^I-rh-Anx5. The radiolabeled protein was rapidly cleared from the blood after a bi-exponential clearance characterized by a rapid phase (t_½α_ = 3.87 ± 0.90 min) and a slow phase (t_½β_ = 4.13 ± 2.04 h). The major organ radioactivity [percent injected dose per gram (%ID/g)] levels (n = 3) at 60 min were 35.37 ± 13.70 (stomach), 21.29 ± 9.97 (kidneys), 12.62 ± 4.27 (bladder), 8.17 ± 2.93 (liver), 7.27 ± 3.66 (spleen), 6.18 ± 1.89 (lungs), 5.91 ± 1.00 (blood), and 0.38 ± 0.09 (brain), At 6 h, the radioactivity levels (%ID/g) were 8.05 ± 0.69 (stomach), 7.71 ± 3.93 (kidneys), 12.62 ± 0.00 (bladder), 4.22 ± 2.01 (liver), 2.38 ± 0.95 (spleen), 2.28 ± 2.41 (lungs), 3.66 ± 3.79 (blood), and 0.34 ± 0.30 (brain), ^123^I-rh-Anx5 was mainly cleared by the kidneys with 86.6% ID of total radioactivity excreted at 48 h.

Lahorte et al. (14) found significantly increased ^123^I-Anx5 radioactivity localization in myocardial apoptosis induced in a rat model of septic shock. Cornelissen et al. (15) also reported that ^123^I-Anx5 could be used to monitor apoptosis induced by farnesyltransferase inhibitors in athymic mice bearing LoVo- human colon adenocarcinoma bearing athymic mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20)]

Tait et al. (13) evaluated ^123^I-Anx5 (obtained from human placenta) as a platelet-directed thrombus targeting agent in a swine model. Fully occluded arterial thrombi were induced in Yorkshire swine. Each swine received 48.1−506.9 MBq (1.3−13.7 mCi) ^123^I-Anx5 (50−500 μg) by i.v. administration. The blood clearance followed a biexponential clearance pattern with an initial rapid phase of t_½_ = 6.4 min and a slow phase with a t_½ =_ 71 min. The combined (60 and 120 min, n = 9) showed that the radioactivity levels (%ID/g) in major organs were 0.1652 ± 0.0511 (kidney), 0.0403 ± 0.0734 (unblocked thyroid), 0.0389 ± 0.0286 (spleen), 0.0169 ± 0.0030 (lung), 0.0072 ± 0.0020 (liver), and 0.0071 ± 0.0088 (carotid artery). The radioactivity levels in the carotid thrombus and femoral thrombus were 0.0482 ± 0.0362 and 0.0466 ± 0.0432, respectively. In comparison, nonspecifically radiolabeled globular protein of comparable size (ovalbumin) had a thrombus radioactivity level of only 0.0059 ± 0.0017% ID/g.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28123I-labelled%20human%20recombinant%20annexin%20V%29%20OR%20%28123I-rh-annexin%20V%29%20OR%20%28123I-Annexin%20V%29%29%20AND%20human)]

Lahorte et al. (2) used SPECT imaging to study the biodistribution and dosimetry of ^123^I-rh-Anx5 in six volunteers. Each volunteer was injected with an i.v. dose of 345 ± 38 MBq (9.3 ± 1.03 mCi) ^123^I-rh-Anx5 (940 μg).The 1-6 h whole-body images showed that most of the radioactivity was distributed in the kidneys, bladder, liver, thyroid (blocked), and stomach. The pattern was consistent with urinary excretion and hepatic uptake of the radiolabeled protein and trapping of free ^123^I− by the stomach. Radioactivity levels in the lungs and brain were relatively low. Using the MIRDOSE program, non-decay-corrected geometric mean time-activity curves of major organs were generated for radiation-absorbed dose estimates. The highest radiation-absorbed dose estimate was found in the blocked thyroid [0.1157 ± 0.0621 mGy/MBq (0.31 ± 0.17 mrad/mCi)] despite pretreatment with lugol. The dose (mGy/MBq) to the kidney was 0.03027 ± 0.00797 (0.082 ± 0.022 mrad/mCi), and the dose to the stomach was 0.00779 ± 0.00207 (0.021 ± 0.0056 mrad/mCi;). The estimated mean effective dose for an adult was 0.0201 ± 0.0100 mSv/MBq (0.057 ± 0.027 mrem/mCi).

## References

1 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
2 Lahorte C.M., van de Wiele C., Bacher K., van den Bossche B., Thierens H., van Belle S., Slegers G., Dierckx R.A. (2003). Biodistribution and dosimetry study of 123I-rh-annexin V in mice and humans. Nucl Med Commun.
3 Bohm I., Schild H. (2003). Apoptosis: the complex scenario for a silent cell death. Mol Imaging Biol.
4 Kerr J.F., Wyllie A.H., Currie A.R. (1972). Apoptosis: a basic biological phenomenon with wide-ranging implications in tissue kinetics. Br J Cancer.
5 Brauer M. (2003). In vivo monitoring of apoptosis. Prog Neuropsychopharmacol Biol Psychiatry.
6 Van de Wiele C., Vermeersch H., Loose D., Signore A., Mertens N., Dierckx R. (2004). Radiolabeled annexin-V for monitoring treatment response in oncology. Cancer Biother Radiopharm.
7 Lahorte C.M., Vanderheyden J.L., Steinmetz N., Van de Wiele C., Dierckx R.A., Slegers G. (2004). Apoptosis-detecting radioligands: current state of the art and future perspectives. Eur J Nucl Med Mol Imaging.
8 Narula J., Kietselaer B., Hofstra L. (2004). Role of molecular imaging in defining and denying death. J Nucl Cardiol.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Boersma H.H., Kietselaer B.L., Stolk L.M., Bennaghmouch A., Hofstra L., Narula J., Heidendal G.A., Reutelingsperger C.P. (2005). Past, present, and future of annexin A5: from protein discovery to clinical applications. J Nucl Med.
11 Dekker B., Keen H., Lyons S., Disley L., Hastings D., Reader A., Ottewell P., Watson A., Zweit J. (2005). MBP-annexin V radiolabeled directly with iodine-124 can be used to image apoptosis in vivo using PET. Nucl Med Biol.
12 Zalutsky M.R., Narula A.S. (1987). A method for the radiohalogenation of proteins resulting in decreased thyroid uptake of radioiodine. Int J Rad Appl Instrum [A].
13 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
14 Lahorte C. Petillot P. Neviere R. Marchetti P. Slegers G. The myocardial uptake of 123I-annexin V is increased in septic rats J Labelled Cpd Radiopharm 2001 44Suppl. 1S430 S432
15 Cornelissen B., Lahorte C., Kersemans V., Capriotti G., Bonanno E., Signore A., Van de Wiele C., Dierckx R.A., Slegers G. (2005). In vivo apoptosis detection with radioiodinated Annexin V in LoVo tumour-bearing mice following Tipifarnib (Zarnestra, R115777) farnesyltransferase inhibitor therapy. Nucl Med Biol.